# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-AB.Fab4D5

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-AB.Fab4D5
Abbreviated name: | ^111^In-DOTA-AB.Fab4D5, ^111^In-AB.Fab4D5
Synonym:
Agent Category: | Antibody and peptide
Target: | EGF HER2 receptor and albumin
Target Category: | Antibody and albumin binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%5BAll%20Fields%5D)]

Epidermal growth factor (EGF) is a cytokine composed of 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF, along with at least seven other growth factors and their transmembrane receptor kinases, play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small cell lung, head and neck, and colon cancers (4-6). High levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed to image human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Albumin is known to accumulate in tumors. Nguyen et al. (17) linked an albumin-binding peptide to the carboxyl end of the heavy chain of trastuzumab Fab (Fab4D5) to form a bifunctional AB.Fab4D5, which is able to bind to HER2 and albumin simultaneously. AB.Fab4D5 was conjugated with ^111^In using 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) as a linker to study its ability for tumor imaging (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20synthesis)]

AB.Fab4D5 was constructed by adding a linker (GGGS) and an albumin-binding peptide (QRLMEDICLPRWGCLWEDDF) to the carboxyl terminus of the heavy chain (18). Fab4D5, AB.Fab4D5, and trastuzumab (10 mg/ml in PBS, 2.5 mM EDTA) were conjugated with 5 mg/ml of DOTA-(N-hydroxysuccinimidyl) ester in N-N'-dimethylacetamide at a 5:1 molar ratio at 30°C for 1 h. Conjugations typically resulted in a ~2 DOTA per protein. ^111^InCl_3_ was mixed with DOTA conjugate in ammonium acetate at 25°C for 1 h. Reactions were quenched with 2 mM diethylenetriaminepentaacetic acid, and ^111^In-DOTA-labeled conjugates were purified using NAP-5 columns. Samples typically contained ~74 MBq/mg protein (2 mCi/mg protein).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20in%20vitro)]

Dennis et al. (18) performed albumin-binding assays with AB.Fab4D5 to displace a biotinylated albumin-binding peptide (SA06b) to prevent binding to rabbit albumin. AB.Fab4D5 and unbiotinylated SA06 displaced SA06b to a similar extent with IC_50_ values of 107 and 65 nM, respectively, whereas Fab4D5 had no effect in this assay. Binding of AB.Fab4D5 to HER2_ecd_ was comparable with Fab4D5 and was unaffected by the presence of rabbit albumin with IC_50_ values of 22 and 15 nM, respectively. Affinity of Fab4D5 for HER2_ecd_ was previously reported as 0.1 nM. Ability of AB.Fab4D5 to bind HER2_ecd_ and albumin simultaneously was shown by binding AB.Fab4D5 to immobilized albumin followed by detection with biotinylated HER2_ecd_. No signal was detected with Fab4D5 in this assay. However, AB.Fab4D5 acts as a bifunctional fusion protein and is able to bind both albumin and HER2_ecd_ simultaneously.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20rodentia)]

Dennis et al. (18) monitored biodistribution by integrated single-photon emission computed tomography/computed tomography analysis in nude mice bearing Fo5 mammary tumors after injection of therapeutic doses of 11.1–18.5 MBq (300–500 μCi) ^111^In-DOTA-labeled conjugates (4 mg/kg). ^111^In-DOTA-Fab4D5 tumor radioactivity was characterized by rapid but transient accumulation in the tumors at 2 h with little retention, followed by rapid accumulation in the kidney by 6 h. ^111^In-DOTA-trastuzumab accumulated slowly in tumors and cleared slowly from normal tissues, although significant tumor accumulation was achieved at 24 h. In contrast, ^111^In-DOTA-AB.Fab4D5 was observed at 2 h in the tumor and gradually leveled at 24 h, similar to ^111^In-DOTA-trastuzumab. Similar tumor accumulation was achieved at 48 h for both ^111^In-DOTA-AB.Fab4D5 and ^111^In-DOTA-trastuzumab (35.9 ± 1.8% and 38.2 ± 3.1% injected dose/g, respectively). However, ^111^In-DOTA-AB.Fab4D5 accumulated in tumors more rapidly and quickly cleared from blood, leading to a lower overall normal tissue background. Importantly, unlike ^111^In-DOTA-Fab4D5, ^111^In-DOTA-AB.Fab4D5 did not accumulate in the kidney, which suggests that association with albumin leads to an altered route of clearance and metabolism. Intravital microscopy at peak tumor accumulation revealed that tumor cell staining by FITC-AB.Fab4D5 was more uniform than for FITC-Fab4D5 or FITC-trastuzumab.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AB.Fab4D5%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Nguyen A., Reyes A.E., Zhang M., McDonald P., Wong W.L., Damico L.A., Dennis M.S. (2006). The pharmacokinetics of an albumin-binding Fab (AB.Fab) can be modulated as a function of affinity for albumin. Protein Eng Des Sel.
18 Dennis M.S., Jin H., Dugger D., Yang R., McFarland L., Ogasawara A., Williams S., Cole M.J., Ross S., Schwall R. (2007). Imaging tumors with an albumin-binding Fab, a novel tumor-targeting agent. Cancer Res.